# [^18^F]-N-{4-[(4,5-Dichloro-2-fluorophenyl)amino]quinazoline-6-yl}-dimethylamine-butylamide

Chemical name: | [^18^F]-N-{4-[(4,5-Dichloro-2-fluorophenyl)amino]quinazoline-6-yl}-dimethylamine-butylamide
Abbreviated name: | [^18^F]ML04
Synonym: | [^18^F]TKS040
Agent Category: | Ligand (irreversible inhibitor)
Target: | Epidermal growth factor receptor tyrosine kinase (EGFR-TK)
Target Category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=egfr+expression+in+cancer)]

The epidermal growth factor receptor (EGFR) mediates its activity through an associated intracellular tyrosine kinase (TK) that controls the signal transduction pathway(s) responsible for the stimulation of cell processes such as growth, proliferation, and motility necessary for the progression of cancers (1). Although constitutive activation of the EGFR or a mutated TK are known to promote the development of various cancers, a characteristic feature of some malignantly transformed cells is the overexpression of EGFR or the receptor ligands that result in a constant activation of the receptor (2). In addition, an overactive TK, due to EGFR activation, a gene mutation, or overexpression, may also provide a stimulus for a ligand-free, and unregulated, initiation of the signal transduction pathway(s). Because of their role in the development of the oncogenic phenotype, the EGFR and its associated TK are respectively targeted with antibodies (http://clinicaltrials.gov/ct2/results?term=EGFR+antibodies) and small molecule inhibitors (http://clinicaltrials.gov/ct2/results?term=EGFR+tyrosine+kinase+inhibitors), respectively0 for the treatment of various cancers (3). Several of these agents are under evaluation in clinical trials (http://clinicaltrials.gov/ct2/results?term=EGFR+inhibitors) approved by the United States Food and Drug Administration. The EGFR-TK inhibitors bind, reversibly or irreversibly, to the intracellular ATP binding site of the enzyme, prevent autophosphorylation of the receptor, and inhibit the signal transduction pathway(s) responsible for initiation of the biological processes mediated by the EGFR (3, 4).

Determination of the EGFR content of cancerous tumors with noninvasive imaging techniques could help monitor cancer patients who are likely to benefit from an anti-EGFR or anti-TK therapy and perhaps predict the treatment prognosis for patients. The use of labeled reversible EGFR-TK inhibitors with positron emission tomography (PET) for the imaging of EGFR was evaluated earlier (5, 6), but these imaging agents were determined to be unsuitable for this purpose because of the high intracellular ATP content that resulted in rapid clearance of the label from the cells, rendering the compounds ineffective for PET imaging of tumors. To alleviate the limitations observed with the reversible TK inhibitor PET probes, investigators developed and evaluated the use of nuclide-labeled irreversible TK inhibitors for the imaging of EGFR (7, 8). Mishani et al. reported that derivatives of the 4-dimethylamino-but-2-enoic acid [4-(phenylamino)-quinazoline-6-yl]-amide group had a high chemical and biological stability as well as high specificity as irreversible inhibitors of the EGFR-TK (9). On the basis of these observations, Abourbeh et al. developed and characterized an ^18^F-labeled PET imaging compound, [^18^F]ML04 (also known as [^18^F]TKS040), for EGFR-TK inhibition under in vitro conditions (10). Abourbeh et al. also studied the biodistribution of this radiochemical in mice bearing EGFR-overexpressing xenograft tumors.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+synthesis)]

ML04 was synthesized as described by Mishani et al. (9). The ^18^F labeling of ML04 to yield [^18^F]ML04 was performed as detailed elsewhere (10). The average radiochemical yield and purity of the tracer was 14% and 98% (n = 10 reactions), respectively, as determined with high-performance liquid chromatography. The total time of radiosynthesis, including purification and formulation, was 4 h. The specific activity of [^18^F]ML04 was reported to be 6.66 TBq/mmol (1,800 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+in+vitro)]

Abourbeh et al. investigated the inhibition of EGFR autophosphorylation by ML04 with human epithelial carcinoma A431 cells (high EGFR expression), human breast carcinoma MDA-MB-468 cells (EGFR overexpression), human lung carcinoma PC10 cells (EGFR overexpression), and human non-small cell lung carcinoma (NSCLC) NIH-H1975 cells (mutant EGFR expression) (10) as described by Mishani et al. (9). The cells were exposed to the inhibitor for 1 h as described, and cell lysates were prepared for analysis. The 50% inhibitory concentration (IC_50_) values of the radiolabel for EGFR autophosphorylation of the A431, MDA-MB-468, PC10, and NIH-H1975 NSCLC cells was reported to be 4–10, 1–5, 10–50, and 25 nM, respectively. Another set of the respective cells was exposed to ML04 for 1 h, and the cells were washed with phosphate-buffered saline. The cells were then incubated in growth medium for 8 h, and the IC_50_ values of EGFR autophosphorylation were determined. The IC_50_ values of the radiolabel were reported to be similar to those given above (10). With results obtained from this study, the investigators concluded that ML04 is an irreversible inhibitor of the EGFR in the respective cells.

In another study, the investigators showed that [^18^F]-ML04 could be used to determine the number of EGFR on A431 cells (10). They reported that on average there were 1.56 ± 0.36 × 10^6^ EGFR per cell (n = 4 determinations), which was close to the numbers reported earlier (1–2 × 10^6^ EGFR per cell) by other investigators (10). However, these investigators cautioned that [^18^F]ML04 was an appropriate tool to determine the number of EGFR on cells only if used at carefully adjusted concentrations.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+rodentia)]

The biodistribution of [^18^F]ML04 was investigated in Nude-Hsd athymic nude-nu mice bearing U87MG.wt EGFR tumors (a human glioma cell line that overexpresses the wild-type EGFR (11)) (10). Mice bearing U187MG tumors, an EGFR-negative human glioma cell line, were used as controls for this study. [^18^F]ML04 was injected into the mice through the lateral tail vein, and blood was drawn from the animals at predetermined time points. The animals were euthanized to excise selected organs to determine the amount of accumulated radioactivity in each organ as a percent of injected dose per gram of tissue (% ID/g). Preliminary experiments showed that the optimal uptake of radioactivity in the various organs and tumors was obtained at 3 h after treatment with the radiotracer. These studies also demonstrated that the two vehicles used (5–10% ethanol/saline (n = 12 animals) and IntraLipid (n = 37 animals)) to administer [^18^F]ML04 to the animals behaved similarly, and no statistical difference was noted in the biodistribution of radioactivity with either vehicle.

Abourbeh et al. compared the uptake of [^18^F]ML04 by U87MG.wt EGFR cell xenograft tumors (n = 15–47 animals/time point) with the uptake by control U138MG xenograft tumors (n = 5–14 mice/time point) (10). Animals in the two groups were injected with [^18^F]ML04 as before and euthanized 120, 180, and 240 min after treatment. The tumors and organs of interest were excised from the animals, and the accumulated radioactivity was determined. Compared with the control tumors (accumulated radioactivity was ~0.65% ID/g at all time points), a significantly higher (statistical P value not reported) amount of radioactivity was reported to have accumulated in the U87MG.wt EGFR tumors at all time points (~1.1% ID/g at 120 min and ~0.8% ID/g at 240 min). Although all other organs from these animals showed a decrease in accumulated label from 120–240 min, the fact that the U138MG tumors maintained a constant level of radioactivity suggested that these tumors had a nondisposable blood pool due to a more necrotic nature compared with the U87MG.wt EGFR tumors.

To determine the target specificity of [^18^F]ML04, Abourbeh et al. performed blocking studies using an excess of unlabelled ML04 (10). Tumor-bearing mice (n = 12 animals) were injected with 5–8 mg ML04/kg body weight 1 h prior to treatment with the tracer. For this study, control animals (n = 54 mice) received only [^18^F]ML04 at the same time as animals with a prior treatment of unlabeled ML04. The animals were euthanized 3 h after injection of the label, and radioactivity accumulated in the various organs, including tumors, was determined as before. An examination of the amount of accumulated radioactivity in various tissues of the two groups of animals revealed that, in general, animals with the unlabeled ML04 treatment had a higher amount (although not statistically significant) of accumulated radioactivity compared with the control animals. However, the tumor/tissue label ratios of the blocked animals were significantly lower (P value not reported) compared with the control animals, indicating a lower accumulation of radioactivity in tumors compared to the other tissues.

With results obtained from the respective biodistribution studies, the investigators concluded that the uptake of radioactivity in the tumors may not be entirely caused by EGFR binding (10). They also concluded that the distribution of [^18^F]ML04 in the various tissues was probably flow-dependent, and a possible change in chemical structure or the route of administration could help improve tissue dispersal of the radioactivity.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+Other+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+Other+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=ML04+Other+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimer]

## References

1 Gunby R.H., Sala E., Tartari C.J., Puttini M., Gambacorti-Passerini C., Mologni L. (2007). Oncogenic fusion tyrosine kinases as molecular targets for anti-cancer therapy. Anticancer Agents Med Chem.
2 Miyamoto S., Fukami T., Yagi H., Kuroki M., Yotsumoto F. (2009). Potential for molecularly targeted therapy against epidermal growth factor receptor ligands. Anticancer Res.
3 Sharma P.S., Sharma R., Tyagi T. (2009). Receptor tyrosine kinase inhibitors as potent weapons in war against cancers. Curr Pharm Des.
4 Linardou H., Dahabreh I.J., Bafaloukos D., Kosmidis P., Murray S. (2009). Somatic EGFR mutations and efficacy of tyrosine kinase inhibitors in NSCLC. Nat Rev Clin Oncol.
5 Fredriksson A., Johnstrom P., Thorell J.O., von Heijne G., Hassan M., Eksborg S., Kogner P., Borgstrom P., Ingvar M., Stone-Elander S. (1999). In vivo evaluation of the biodistribution of 11C-labeled PD153035 in rats without and with neuroblastoma implants. Life Sci.
6 Bonasera T.A., Ortu G., Rozen Y., Krais R., Freedman N.M., Chisin R., Gazit A., Levitzki A., Mishani E. (2001). Potential (18)F-labeled biomarkers for epidermal growth factor receptor tyrosine kinase. Nucl Med Biol.
7 Ortu G., Ben-David I., Rozen Y., Freedman N.M., Chisin R., Levitzki A., Mishani E. (2002). Labeled EGFr-TK irreversible inhibitor (ML03): in vitro and in vivo properties, potential as PET biomarker for cancer and feasibility as anticancer drug. Int J Cancer.
8 Mishani E., Abourbeh G., Rozen Y., Jacobson O., Laky D., Ben David I., Levitzki A., Shaul M. (2004). Novel carbon-11 labeled 4-dimethylamino-but-2-enoic acid [4-(phenylamino)-quinazoline-6-yl]-amides: potential PET bioprobes for molecular imaging of EGFR-positive tumors. Nucl Med Biol.
9 Mishani E., Abourbeh G., Jacobson O., Dissoki S., Ben Daniel R., Rozen Y., Shaul M., Levitzki A. (2005). High-affinity epidermal growth factor receptor (EGFR) irreversible inhibitors with diminished chemical reactivities as positron emission tomography (PET)-imaging agent candidates of EGFR overexpressing tumors. J Med Chem.
10 Abourbeh G., Dissoki S., Jacobson O., Litchi A., Ben Daniel R., Laki D., Levitzki A., Mishani E. (2007). Evaluation of radiolabeled ML04, a putative irreversible inhibitor of epidermal growth factor receptor, as a bioprobe for PET imaging of EGFR-overexpressing tumors. Nucl Med Biol.
11 Huang H.S., Nagane M., Klingbeil C.K., Lin H., Nishikawa R., Ji X.D., Huang C.M., Gill G.N., Wiley H.S., Cavenee W.K. (1997). The enhanced tumorigenic activity of a mutant epidermal growth factor receptor common in human cancers is mediated by threshold levels of constitutive tyrosine phosphorylation and unattenuated signaling. J Biol Chem.